# (+/-)-2-(N-Cyclohexylethyl-N-[^11^C]propyl)amino-5-hydroxytetralin

Chemical name: | (+/-)-2-(N-Cyclohexylethyl-N-[^11^C]propyl)amino-5-hydroxytetralin
Abbreviated name: | [^11^C]ZYY-339
Synonym:
Agent Category: | Compound
Target: | D_2_ and D_3_ dopamine receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20ZYY%5BAll%20Fields%5D)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five dopamine receptor subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_). D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system levels. Most striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons.

Dopamine receptors are G-protein–coupled receptors that exist in high- and low-affinity states with respect to agonist binding. The two states are inter-convertible. In the high-affinity state, dopamine receptors are coupled to G-proteins, whereas in the low-affinity state they are not. Dopamine has a dissociation constant (K_d_) of 7 nM for the high-affinity state (K_high_) and a K_d_ of 1,720 nM for the low-affinity state (K_low_) (5). Under physiologic conditions, dopamine binds predominately to receptors in the high-affinity state. The high-affinity state was suggested to be the functional form of the dopamine receptors (6).

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2/3_ receptors, making study of extrastriatal D_2/3_ receptors difficult (7-9). In binding studies, [^123^I]epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2/3_ receptors (10). Epidepride exhibits marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective high-affinity antagonist of D_2/3_ receptors (11), and in positron emission tomography (PET) in vivo studies (12-14) it identified extrastriatal D_2/3_ receptors. However, none of these antagonists distinguishes between the high- and low-affinity states of the D_2_ receptors. Many effects have been pursued to develop radiolabeled agonists for the non-invasive study of the high-affinity state of the D_2/3_ receptors in the brain. (–)-N-[^11^C]Propyl-norapomorphine ([^11^C]NPA) and [^11^C](+)-4-N-propyl-,3,4,4a,5,6,10b-hexahydro-2H-naphth[1,2-b][1,4]-oxazin-9-ol ([^11^C]PHNO) have been studied as radiolabeled dopamine agonists.

Various hydroxytetralin analogs with different binding affinities for the D_2_ receptors have been evaluated as agonist radiotracers (15). (+/-)-2-(N-Cyclohexylethyl-N-[^11^C]propyl)amino-5-hydroxytetralin ([^11^C]ZYY-339) is being developed as a PET agent for the high-affinity states of D_2/3_ receptors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20ZYY%20and%20synthesis)]

Shi et al. (15) reported a two-step synthesis of [^11^C]ZYY-339 in which [^11^C]propionyl chloride was reacted with 5-hydroxy-2-[N-(2-cyclohexylethyl)amino]tetralin and followed by LiAlH_4_ reduction, with a radiochemical yield of 5–10% (based on [^11^C]CO_2_ at the end of bombardment) and an average specific activity of 9–37 GBq/μmol (250–1,000 mCi/μmol) at end of synthesis after purification by high-performance liquid chromatography. [^11^C]Propionyl chloride was prepared by reacting [^11^C]CO_2_ with ethylmagnesium bromide, followed by reaction with phthaloyl chloride. Total synthesis time was 60–75 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20ZYY%20and%20in%20vitro)]

In a binding study of dopamine receptors in membranes of the rat striata with [^3^H]spiperone, ZYY-339 had an IC_50_ of 0.01 nM (15). In vitro autoradiography studies of rat brain slices indicated selective binding of [^11^C]ZYY-339 to the striata, which was completely inhibited by co-incubation with 10 μM sulpride (a D_2/3_ antagonist). Gpp(NH)p decreased the striata/cerebellum ratio from 1.8 to 1.1 by converting the high-affinity states to low-affinity states. There was significant nonspecific binding in the cortex.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20ZYY%20and%20rodentia)]

Biodistribution studies in rats showed a marked accumulation of the tracer in the striata within the first 2 min [1.4% injected dose per gram (ID/g)], followed by a decrease of radioactivity to 0.5% ID/g at 30 min and 0.2% ID/g at 60 min (16). The striata/cerebellum ratios were 1.47 at 2 min, 1.98 at 30 min, and 1.67 at 60 min after injection. Haloperidol pretreatment (1 mg/kg, 15 min before radiotracer injection) effectively reduced specific binding of [^11^C]ZYY-339 to the striata with some residual binding relative to the cerebellum at 30 min. Little inhibition was seen in the cerebellum. [^11^C]ZYY-339 thus displays uptake and washout kinetics characteristic of reversible radiotracers.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20ZYY%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20ZYY%20and%20monkey)]

Mukherjee et al. (16) showed selective accumulation (0.03% ID/ml) in the striata of two rhesus monkeys with striata/cerebellum ratios of 1.4 at 30 min and 1.3 at 60 min after injection of 26–93 MBq (0.7–2.5 mCi) of [^11^C]ZYY-339. Thalamus/cerebellum ratios were 1.3 at 30 min and 1.2 at 60 min. However, there was substantial nonspecific binding in the cortex and cerebellum. The authors suggested that the use of the more active isomer may provide higher striata/cerebellum and thalamus/cerebellum ratios.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20ZYY%20and%20human)]

No relevant publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Sunahara R.K., Guan H.C., O'Dowd B.F., Seeman P., Laurier L.G., Ng G., George S.R., Torchia J., Van Tol H.H., Niznik H.B. (1991). Cloning of the gene for a human dopamine D5 receptor with higher affinity for dopamine than D1. Nature.
6 Sibley D.R., De Lean A., Creese I. (1982). Anterior pituitary dopamine receptors. Demonstration of interconvertible high and low affinity states of the D-2 dopamine receptor. J Biol Chem.
7 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
8 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
9 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
10 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
11 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
12 Grunder G., Landvogt C., Vernaleken I., Buchholz H.G., Ondracek J., Siessmeier T., Hartter S., Schreckenberger M., Stoeter P., Hiemke C., Rosch F., Wong D.F., Bartenstein P. (2005). and , The Striatal and Extrastriatal D2/D3 Receptor-Binding Profile of Clozapine in Patients with Schizophrenia. Neuropsychopharmacology.
13 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
14 Kessler R.M., Ansari M.S., Riccardi P., Li R., Jayathilake K., Dawant B., Meltzer H.Y. (2005). Occupancy of striatal and extrastriatal dopamine d(2)/d(3) receptors by olanzapine and haloperidol. Neuropsychopharmacology.
15 Shi B., Narayanan T.K., Yang Z.Y., Christian B.T., Mukherjee J. (1999). Radiosynthesis and in vitro evaluation of 2-(N-alkyl-N-1'-11C-propyl)amino-5-hydroxytetralin analogs as high affinity agonists for dopamine D-2 receptors. Nucl Med Biol.
16 Mukherjee J., Narayanan T.K., Christian B.T., Shi B., Yang Z.Y. (2004). Binding characteristics of high-affinity dopamine D2/D3 receptor agonists, 11C-PPHT and 11C-ZYY-339 in rodents and imaging in non-human primates by PET. Synapse.